# ^68^Ga-1,4,7,10-Tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-aminohexanoic acid-Lys^40^-exendin-4

Chemical name: | ^68^Ga-1,4,7,10-Tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-aminohexanoic acid-Lys^40^-exendin-4
Abbreviated name: | [Lys^40^(Ahx-DOTA-^68^Ga)NH_2_]-exendin-4
Synonym: | ^68^Ga-DOTA-Ahx-Lys^40^-exendin-4
Agent category: | Peptide
Target: | Glucagon-like peptide-1 receptor (GLP-1R)
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^68^Ga
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=248418), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&val=1916066) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=14526) for more information about exendin-4.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=68Ga%20Exendin-4)]

Glucagon-like peptide-1 (GLP-1, 30 amino acids) is secreted from enteroendocrine cells of the distal small intestine in response to food ingestion (1). GLP-1 plays an important role in glucose metabolism and homeostasis. It inhibits gastric emptying, glucagon secretion, and glucose production (2). In addition, it induces insulin release from the pancreatic β-cells as well as their proliferation. The GLP-1 receptor has been identified in normal tissues such as the pancreas, stomach, brain, and lung, and it has been shown to be highly overexpressed in human insulinomas and gastrinomas (3). In insulinomas, GLP-1 receptor density is considerably greater, and the GLP-1 receptor is more frequently observed than somatostatin receptors.

Exendin-4 is a GLP-1 analog with 39 amino acids isolated from the venom of the Gila monster (Heloderma suspectum) (4). Exendin-4 and GLP-1 share a 53% amino acid sequence homology. Exendin-4 is a more potent and longer-lasting GLP-1 receptor agonist than GLP-1. Exendin-4 is resistant to cleavage by dipeptidyl peptidase IV, whereas the first two N-terminal amino acids of GLP-1 are rapidly cleaved. Exenatide, a synthetic version of exendin-4, is the first GLP-1 mimetic recently approved by the United States Food and Drug Administration (FDA) for use in select patients with type 2 diabetes (5). ^68^Ga-1,4,7,10-Tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-aminohexanoic acid-Lys^40^-exendin-4 ([Lys^40^(Ahx-DOTA-^68^Ga)NH_2_]-exendin-4) is being developed for positron emission tomography (PET) imaging of the GLP-1 receptor (6).

### Related Resource Links:

- Chapters in MICAD (GLP-1 (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=GLP-1%5BAll+Fields%5D+AND+micad%5Bbook%5D))
- Gene information in NCBI (GLP-1R (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=DetailsSearch&Term=2740))
- Articles in Online Mendelian Inheritance in Man (OMIM) (GLP-1R (http://omim.org/entry/138032))
- Clinical trials (Exendin (http://www.clinicaltrials.gov/ct2/results?term=GLP-1))
- Drug information in FDA (Exendin (http://google2.fda.gov/search?q=exendin&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=11&y=18))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=68Ga%20Exendin-4%20and%20synthesis)]

The structure and composition of [Lys^40^(Ahx-DOTA)NH_2_]-exendin-4 was verified with high-performance liquid chromatography and matrix-assisted laser desorption-ionization mass spectrometry (6). A mixture of ^68^GaCl_3_ and [Lys^40^(Ahx-DOTA)NH_2_]-exendin-4 was incubated in HEPES buffer (pH, 3.6) for 5 min at 95°C with a >98% labeling yield of [Lys^40^(Ahx-DOTA-^68^Ga)NH_2_]-exendin-4 and a specific activity of 13 GBq/µmol (0.35 Ci/µmol). The stability of [Lys^40^(Ahx-DOTA-^68^Ga)NH_2_]-exendin-4 in solution was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=68Ga%20Exendin-4%20and%20in%20vitro)]

Wild et al. (6) reported that [Lys^40^(Ahx-DOTA-^68^Ga)NH_2_]-exendin-4 was specifically accumulated into β-cell tumors in culture with 2.48 ± 0.29% of incubation dose at 1 h and 10.35 ± 0.43% at 4 h. Most of the accumulated radioactivity was internalized into the cells (>80%).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=68Ga%20Exendin-4%20and%20rodentia)]

Wild et al. (6) performed ex vivo biodistribution studies with the use of Rip1Tag2 mice (n = 6/group) with spontaneous insulinoma β-cell tumors. The organ with the highest uptake was the tumor (205 ± 59% injected dose/g (% ID/g)), followed by the kidneys (202 ± 34% ID/g), lungs (43 ± 5% ID/g), pancreas (14 ± 1% ID/g), spleen (2.3 ± 0.6% ID/g), stomach (2.1 ± 0.8% ID/g), and liver (0.6 ± 0.1% ID/g) at 4 h after injection of [Lys^40^(Ahx-DOTA-^68^Ga)NH_2_]-exendin-4 (10 pmol/mouse). Excess unlabeled [Lys^40^(Ahx-DOTA)NH_2_]-exendin-4 (5 nmol) blocked accumulation by >95% in the tumor and GLP-1R-expressing organs, such as the pancreas and lung, but there was little inhibition in the kidneys. Blood clearance was fast, with 0.3% ID/g remaining in the blood 4 h after injection. In contrast, the tumor washout rate was slow. The tumor/blood ratio was 89 at 0.5 h and 706 at 4 h. The tumor/muscle, tumor/pancreas, and tumor/kidney ratios were 205, 15, and 1 at 4 h, respectively.

PET imaging in one Rip1Tag2 mouse identified high uptake in the kidneys at 1 h after injection of 0.13 MBq (0.0035 mCi) [Lys^40^(Ahx-DOTA-^68^Ga)NH_2_]-exendin-4. After bilateral nephrectomy, PET imaging clearly identified two tumors (1.5 mm and 2.3 mm) in the pancreas. No blocking studies were reported.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=68Ga%20Exendin-4%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=68Ga%20Exendin-4%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed] (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=68Ga%20Exendin-4%20and%20human)

No publication is currently available.

## References

1 Theodorakis M.J., Carlson O., Michopoulos S., Doyle M.E., Juhaszova M., Petraki K., Egan J.M. (2006). Human duodenal enteroendocrine cells: source of both incretin peptides, GLP-1 and GIP. Am J Physiol Endocrinol Metab.
2 Doyle M.E., Egan J.M. (2001). Glucagon-like peptide-1. Recent Prog Horm Res.
3 Reubi J.C., Waser B. (2003). Concomitant expression of several peptide receptors in neuroendocrine tumours: molecular basis for in vivo multireceptor tumour targeting. Eur J Nucl Med Mol Imaging.
4 Meier J.J., Nauck M.A. (2005). Glucagon-like peptide 1(GLP-1) in biology and pathology. Diabetes Metab Res Rev.
5 Nielsen L.L., Young A.A., Parkes D.G. (2004). Pharmacology of exenatide (synthetic exendin-4): a potential therapeutic for improved glycemic control of type 2 diabetes. Regul Pept.
6 Wild D., Wicki A., Mansi R., Behe M., Keil B., Bernhardt P., Christofori G., Ell P.J., Macke H.R. (2010). Exendin-4-based radiopharmaceuticals for glucagonlike peptide-1 receptor PET/CT and SPECT/CT. J Nucl Med.